# Trastuzumab-manganese–doped iron oxide nanoparticles

Chemical name: | Trastuzumab-manganese–doped iron oxide nanoparticles
Abbreviated name: | Trast-MnMEIO nanoparticles
Synonym: | MnMEIO-Herceptin
Agent Category: | Antibody
Target: | EGF HER2 receptor
Target Category: | Antibody binding to EGF receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MEIO%20and%20HER2)]

Epidermal growth factor (EGF) is a cytokine (6.2 kDa) composed of 53 amino acids that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non–small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxide particles are coated with a protective layer of dextran or other polysaccharide. These particles have large combined magnetic moments or spins that are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in magnetic resonance (MR) imaging, though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into the reticuloendothelial system (RES) is by endocytosis or phagocytosis. SPIO particles are taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells (11). SPIO agents are classified by their sizes with coating material (~20 nm to 3,500 nm in diameters) as large SPIO (LSPIO) nanoparticles, standard SPIO (SSPIO) nanoparticles, ultrasmall SPIO (USPIO) nanoparticles, and cross-linked iron oxide nanoparticles (CLIO). A new class of iron oxide nanoparticles has been created with high and tunable nanomagnetism: magnetism-engineered iron oxide (MEIO) nanoparticles (12). These MEIO nanoparticles were doped with manganese (MnMEIO) to provide further MR signal enhancement.

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (13). Cardiotoxicity is the most serious complication of trastuzumab use in humans with breast cancer (14). One potential application of a radiolabeled anti-HER2 mAb is pretreatment imaging of breast cancer patients to predict the therapeutic efficacy of trastuzumab. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (15-19). Trastuzumab has also been successfully coupled with MnMEIO nanoparticles to study MR imaging of HER2 in tumors in mice (12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MEIO%20and%20HER2%20and%20engineered)]

Lee et al. (12) prepared MnMEIO nanoparticels by means of a high-temperature nonhydrolytic reaction between MnCl2 and iron tris-2,4-pentadionate in the presence of oleic acid and oleylamine as surfactants. MnMEIO nanoparticles were then coated with 2,3-dimercaptosuccinic acid molecules.MnMEIO nanoparticles (~12 nm in diameter) exhibited a high mass magnetization of 110 emu/mass of magnetic atoms with a high magnetic spin of 5 μ_B_ and a high R2 relaxivity value (R2 = 1/T2) of 358 liters/mmol/s. Trastuzumab (2 mg) was first activated with the heterobifunctional cross-linker sulfo-succinimidyl-4-(maleimidomethyl)-1-cyclohexanecarboxylate to yield maleimide-activated trastuzumab. MnMEIO nanoparticles (0.2 mg Fe) were mixed with the maleimide-activated trastuzumab for 8 h at 4°C. Trastuzumab-conjugated MnMEIO (trast-MnMEIO) nanoparticles were purified by gel filtration. There were ~6 antibodies/nanoparticle.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MEIO%20and%20HER2%20and%20in%20vitro)]

Lee et al. (12) performed cell-binding assays with trast-MnMEIO nanoparticles using various cell lines with different levels of HER2/neu overexpression: Bx-PC-3, MDA-MB-231, MCF-7, and NIH3T6.7 (relative HER2/neu expression levels are 1, 3, 28, and 2,300, respectively) with R2 enhancement of 10%, 40%, 70%, and 130%, respectively. Trastuzumab-MEIO conjugates exhibited R2 relaxivity enhancements of 8%, 18%, 29%, and 52% for Bx-PC-3, MDA-MB-231, MCF-7, and NIH3T6.7 cell lines, respectively. On the other hand, binding of trastuzumab-CLIO nanoparticles was negligible in all cell lines with only 10% R2 enhancement in NIH3T6.7 cells. Fluorescence flow cytometry showed that nearly identical numbers of MnMEIO and CLIO nanoparticles were bound to each cell line. The observed high MR enhancement effect of MnMEIO seems to be attributable to the fact that its R2 relaxivity coefficient per nanoparticle is much higher than that of CLIO. No blocking experiment was performed.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MEIO%20and%20HER2%20and%20rodentia)]

Lee et al. (12) studied the accumulation of trast-MnMEIO nanoparticles in nude mice bearing NIH3T6.7 tumors (n = 8) using a 1.5 T clinical MR imaging system before and after injection of trast-MnMEIO (20 mg/kg). The small tumors (~50 mg) were clearly delineated at 1 h (25% R2 increase) and 2 h (34% R2 increase) after injection. In contrast, trastuzumab-CLIO (20 mg/kg) showed only a <5% R2 increase, and trastuzumab-MEIO (20 mg/kg) showed only a 10% R2 increase. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MEIO%20and%20HER2%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MEIO%20and%20HER2%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MEIO%20and%20HER2%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
12 Lee J.H., Huh Y.M., Jun Y.W., Seo J.W., Jang J.T., Song H.T., Kim S., Cho E.J., Yoon H.G., Suh J.S., Cheon J. (2007). Artificially engineered magnetic nanoparticles for ultra-sensitive molecular imaging. Nat Med.
13 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
14 Goldenberg M.M. (1999). Trastuzumab, a recombinant DNA-derived humanized monoclonal antibody, a novel agent for the treatment of metastatic breast cancer. Clin Ther.
15 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
16 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
17 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
18 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
19 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.